# ^86^Y-CHX-A”-Rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_

Chemical name: | ^86^Y-CHX-Rhenium-cyclized-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_
Abbreviated name: | ^86^Y-CHX-A”-ReCCMSH(Arg^11^)
Synonym:
Agent category: | Peptide
Target: | Melanocortin-1 (MC-1) receptor (MC1R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^86^Y
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=27477129), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=27477128) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=4157&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about the Melanocortin-1 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH)]

Malignant melanoma is the most deadly form of skin cancer (1). Early and accurate diagnosis is necessary for surgery and successful treatment (2). The melanocortin (MC) system is a neuropeptide network of the skin, and it is involved in pigmentation regulation, cortisol production, and many other physiological processes (3). Most cutaneous cell types express MC receptors, pro-opiomelanocortin (POMC), and prohormone convertases, and they also release MCs. Melanotropin-stimulating hormones (α-, β-, and γ-MSH) are derived from POMC by the proteolytic action of prohormone convertases. There are five MC receptors (MC1R to MC5R), which belong to the G-protein−coupled receptor superfamily, and these receptors have been found to be overexpressed in melanoma cells (4, 5). α-MSH (Ac-Ser^1^-Tyr^2^-Ser^3^-Met^4^-Glu^5^-His^6^-Phe^7^-Arg^8^-Trp^9^-Gly^10^-Lys^11^-Pro^12^-Val^13^-NH_2_), produced by the brain and the pituitary gland, is a tridecapeptide (13 amino acids) and is the most potent melanotropic peptide (6) in the regulation of skin pigmentation via MC1R.

Positron emission tomography (PET) imaging with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) in cancer has been approved by United States Food and Drug Administration with many on-going clinical trials. Although [^18^F]FDG is effective in the detection of melanoma, it is not melanoma-specific and some melanoma cells do not take up [^18^F]FDG (7, 8). Radiolabeled α-MSH peptide analogs have been shown to specifically bind to MC1R that is overexpressed on human and mouse melanoma cells (4, 5, 7, 9, 10). N-(2-Aminoethyl)-trans-1,2-diaminocyclohexane-N,N”,N”’-pentaacetic acid (CHX-A”) has been successfully coupled to α-MSH peptide analogs for radiolabeling with a variety of radionuclides (7, 11, 12). A rhenium-cyclized α-MSH analog, Re-[Cys^3,4,10^,D-Phe^7^,Arg^11^]α-MSH_3-13_ (ReCCMSH(Arg^11^)), was conjugated with CHX-A” (CHX-A”-ReCCMSH(Arg^11^)) and radiolabeled with ^86^Y (^86^Y-CHX-A”-ReCCMSH(Arg^11^)) as a potential molecular imaging agent to target melanoma (13). Rhenium-mediated cyclization exhibits significantly reduced nonspecific renal radioactivity accumulation high tumor uptake and retention coupled with rapid clearance kinetics, compared with its free sulfhydryl and disulfide bond–containing counterparts (10). ^86^Y is a positron emitter with a physical half-life of 14.7 h and is suitable for PET imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+and+synthesis)]

Wei et al. (13) reported the synthesis of ^86^Y-CHX-A”-ReCCMSH(Arg^11^). The CCMSH(Arg^11^) peptide was synthesized using standard Fmoc chemistry on an amide resin with a peptide synthesizer. CCMSH(Arg^11^) was then reacted with 2 M excess of the glutaric acid succinimidyl ester derivative of CHX-A” to the N-terminus of CCMSH(Arg^11^) to form CHX-A”-CCMSH(Arg^11^). A mixture of CHX-A”-CCMSH(Arg^11^) and ReOCl_3_ (1:1.5 molar ratio) was incubated for 30 min at 85°C. The cyclized peptide, CHX-A”-ReCCMSH(Arg^11^), was purified with high-performance liquid chromatography. For ^86^Y labeling, a solution of ^86^Y and CHX-A”-ReCCMSH(Arg^11^) was heated for 30 min at 75°C. Radiochemical efficiency was reported to be >95% with a specific activity of 8.77 GBq/µmol (237 mCi/µmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+in+vitro)]

Chen et al. (10) determined the 50% inhibition concentration (IC_50_) value of DOTA-ReCCMSH(Arg^11^) to be 1.2 ± 0.3 nM using B16/F1 murine melanoma cells with ^125^I-(Tyr^2^)-[Nle^4^, D-Phe]α-MSH (^125^I-NDP). In comparison, the IC_50_ value of ReCCMSH(Arg^11^) was 2.9 ± 0.3 nM. Wei et al. (13) found that the IC_50_ value for CHX-A”-ReCCMSH(Arg^11^) was 3.8 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+rodentia)]

Wei et al. (13) performed biodistribution studies in female C57BL/6 mice (n = 5/group) bearing 10-day-old B16/F1 murine melanoma tumors. Each mouse received 0.3 MBq (0.008 mCi, 35 pmol) ^86^Y-CHX-A”-ReCCMSH(Arg^11^). The tumor uptake radioactivity levels were obtained at 30 min, 2 h, 4 h, and 24 h, respectively: 3.99 ± 0.54% injected dose per gram (% ID/g), 4.68 ± 1.02% ID/g, 4.18 ± 0.45% ID/g, and 2.79 ± 0.44% ID/g. The tumor retention was high up to 4 h after injection. Pretreatment with 9 nmol unlabeled NDP significantly reduced the tumor uptake to 2.1 ± 0.46% ID/g (P < 0.02) at 2 h after injection. No other tissues showed significant inhibition by NDP. The ^86^Y-CHX-A”-ReCCMSH(Arg^11^) uptake in nontarget tissue (except the kidneys and liver) was low at 2 h. Furthermore, the radioactivity was quickly cleared from most of the tissues (except the kidneys and liver) at 2 h after injection (e.g., kidney: 10.95 ± 3.01% ID/g at 30 min and 8.1 ± 3.62% ID/g at 2 h; liver: 4.23 ± 0.36% ID/g at 30 min and 3.30 ± 0.54% ID/g at 2 h; blood: 4.65 ± 0.98% ID/g at 30 min and 1.09 ± 0.24% ID/g at 2 h; lung: 3.44 ± 0.43% ID/g at 30 min and 1.24 ± 0.18% ID/g at 2 h). The tumor/muscle and tumor/blood ratios at 2 h were 20 and 4, respectively. PET imaging of mice bearing the B16/F1 melanoma tumors was conducted at 2 h after intravenous injection of 13 MBq (0.35 mCi) ^86^Y-CHX-A”-ReCCMSH(Arg^11^). The tumor, urinary bladder, and kidneys were clearly visible. Preinjection of 9 nmol unlabeled NDP inhibited the tumor accumulation, whereas there was little inhibition of radioactivity in the kidneys. In comparison with ^111^In- and ^68^Ga-CHX-A”-ReCCMSH(Arg^11^), ^86^Y-CHX-A”-ReCCMSH(Arg^11^) exhibited higher liver accumulation. ^111^In- and ^86^Y-CHX-A”-ReCCMSH(Arg^11^) showed higher tumor accumulation than ^68^Ga-CHX-A”-ReCCMSH(Arg^11^), which has a lower specific activity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CCMSH+AND+human)]

No publication is currently available.

## NIH Support

Intramural Research Program, R24 CA86307, R24 CA86060, P30 CA91842

## References

1 Jemal A., Siegel R., Ward E., Murray T., Xu J., Thun M.J. (2007). Cancer statistics, 2007. CA Cancer J Clin.
2 Miao Y., Hylarides M., Fisher D.R., Shelton T., Moore H., Wester D.W., Fritzberg A.R., Winkelmann C.T., Hoffman T., Quinn T.P. (2005). Melanoma therapy via peptide-targeted {alpha}-radiation. Clin Cancer Res.
3 Bohm M., Luger T.A., Tobin D.J., Garcia-Borron J.C. (2006). Melanocortin receptor ligands: new horizons for skin biology and clinical dermatology. J Invest Dermatol.
4 Miao Y., Whitener D., Feng W., Owen N.K., Chen J., Quinn T.P. (2003). Evaluation of the human melanoma targeting properties of radiolabeled alpha-melanocyte stimulating hormone peptide analogues. Bioconjug Chem.
5 Siegrist W., Solca F., Stutz S., Giuffre L., Carrel S., Girard J., Eberle A.N. (1989). Characterization of receptors for alpha-melanocyte-stimulating hormone on human melanoma cells. Cancer Res.
6 Catania A., Airaghi L., Garofalo L., Cutuli M., Lipton J.M. (1998). The neuropeptide alpha-MSH in HIV infection and other disorders in humans. Ann N Y Acad Sci.
7 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
8 Dimitrakopoulou-Strauss A., Strauss L.G., Burger C. (2001). Quantitative PET studies in pretreated melanoma patients: a comparison of 6-[18F]fluoro-L-dopa with 18F-FDG and (15)O-water using compartment and noncompartment analysis. J Nucl Med.
9 Tatro J.B., Reichlin S. (1987). Specific receptors for alpha-melanocyte-stimulating hormone are widely distributed in tissues of rodents. Endocrinology.
10 Chen J., Cheng Z., Owen N.K., Hoffman T.J., Miao Y., Jurisson S.S., Quinn T.P. (2001). Evaluation of an (111)In-DOTA-rhenium cyclized alpha-MSH analog: a novel cyclic-peptide analog with improved tumor-targeting properties. J Nucl Med.
11 Wei L., Butcher C., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Lewis J.S. (2007). Synthesis and biologic evaluation of 64Cu-labeled rhenium-cyclized alpha-MSH peptide analog using a cross-bridged cyclam chelator. J Nucl Med.
12 Wei L., Miao Y., Gallazzi F., Quinn T.P., Welch M.J., Vavere A.L., Lewis J.S. (2007). Gallium-68-labeled DOTA-rhenium-cyclized alpha-melanocyte-stimulating hormone analog for imaging of malignant melanoma. Nucl Med Biol.
13 Wei L., Zhang X., Gallazzi F., Miao Y., Jin X., Brechbiel M.W., Xu H., Clifford T., Welch M.J., Lewis J.S., Quinn T.P. (2009). Melanoma imaging using 111In-, 86Y- and 68Ga-labeled CHX-A''-Re(Arg11)CCMSH. Nucl Med Biol.